# ^18^F-Labeled N-succinimidyl-4-fluorobenzoate–conjugated rat anti-mouse vascular endothelial growth factor receptor 2 monoclonal antibody linked to microbubbles

Chemical name: | ^18^F-Labeled N-succinimidyl-4-fluorobenzoate–conjugated rat anti-mouse vascular endothelial growth factor receptor 2 monoclonal antibody linked to microbubbles
Abbreviated name: | [^18^F]-4SFB-Avas12a1 MB
Synonym:
Agent Category: | Antibody
Target: | Vascular endothelial growth factor receptor 2
Target Category: | Receptor
Method of detection: | Positron emission tomography (PET)
Source of signal / contrast: | ^18^F
Activation: | No
Studies: | - In vitro; - Rodents | Structure not available in PubChem (http://pubchem.ncbi.nlm.nih.gov/).

## Background

[PubMed (http://www.ncbi.nlm.nih.gov/pubmed?term=VEGFR2%20Targeted%20microbubbles&cmd=DetailsSearch)]

Microbubbles (MBs) are spherical shells that are made of various types of biocompatible materials, such as albumin, carbohydrates, lipids or polymers, and are filled with heavy gases (nitrogen, perfluorocarbon, or sulfur hexafluoride) in the core. In the clinic, MBs are commonly used for the noninvasive real-time imaging of inflammation, thrombus formation, and angiogenesis with ultrasonography (1, 2). The features and utility of MBs have been discussed recently by Postema and Gilja (3). Targeted MBs can be generated by coating the MB shells with small molecules, peptides, proteins, or antibodies (Abs) that have a high binding affinity for disease-specific molecular markers, such as α_V_β_3_ integrins, endoglin, and the vascular endothelial growth factor receptor 2 (VEGFR2), which are expressed on the surface of endothelial cells (2). Because MBs are inexpensive, widely available, and easy to use, there is much interest in the preclinical development and evaluation of targeted MBs for the imaging of diseases related to the circulatory system (4). Investigators are particularly interested in targeting the VEGFR2 with MBs because, once activated, this receptor initiates several signal transduction pathways that influence the differentiation, mitogenic potential, and migration of the endothelial cells, and VEGFR2 is overexpressed in cancerous tumors to promote angiogenesis in the lesions. In addition, VEGFR2 is the target of several antiangiogenic drugs that have been approved by the United States Food and Drug Administration for the treatment of various cancers (e.g., bevacizumab (http://dailymed.nlm.nih.gov/dailymed/lookup.cfm?setid=939b5d1f-9fb2-4499-80ef-0607aa6b114e), an anti-VEGFR2 Ab). It was shown in a preclinical study that MBs coated with a rat anti-mouse VEGFR2 Ab (Avas12a1 MBs) can be used with ultrasonography imaging to visualize tumor angiogenesis in mice, but the biodistribution of the targeted MBs was not investigated (5). However, it is important to study the biodistribution of a therapeutic drug or an imaging agent because such investigations are essential to determine the pharmacokinetics, nonspecific targets, and side effects of a drug or imaging agent. Therefore, in continuation of the earlier study (5), the biodistribution of ^18^F-labeled Avas12a1 MBs was investigated with dynamic micro-positron emission tomography (micro-PET) in mice bearing mouse angiosarcoma SVR (http://www.atcc.org/ATCCAdvancedCatalogSearch/ProductDetails/tabid/452/Default.aspx?ATCCNum=CRL-2280&Template=cellBiology) cell tumors (2).

### Related Resource Links

VEGFR2-related chapters in MICAD (http://www.ncbi.nlm.nih.gov/books/?term=VEGFR+2+AND+micad%5Bbook%5D&view=chapter&p%24a=&p%24l=PBooksLayout&p%24st=books)

Human VEGFR, variant 1, protein and mRNA sequences (http://www.ncbi.nlm.nih.gov/nuccore/NM_002019.4)

Clinical trials (http://clinicaltrials.gov/ct2/results?term=VEGFR) related to VEGFR

VEGF and VEGFR signaling network (http://pid.nci.nih.gov/search/pathway_landing.shtml?what=graphic&jpg=on&pathway_id=200107&source=NATURE&output-format=graphic&ppage=1&genes_a=3791) (from Pathways Interaction Database)

United States Food and Drug Administration approved anti-VEGFR2 drugs (http://dailymed.nlm.nih.gov/dailymed/search.cfm?startswith=Vascular+endothelial+growth+factor+receptor)

## Synthesis

[PubMed (http://www.ncbi.nlm.nih.gov/pubmed?term=MBs%20targeted%20to%20VEGFR2%20synthesis&cmd=DetailsSearch)]

The MBs (lipid shells containing perfluorocarbon) and the rat anti-mouse VEGFR2 Ab used in the different studies were obtained from commercial sources (2). Initially ^18^F-labeled N-succinimidyl 4-fluorobenzoate ([^18^F]-4SFB; specific activity 200–250 GBq/μmol (5.4–6.75 Ci/μmol)) was conjugated to Avas12a1, and the radiolabeled Ab was then used to coat the MBs for the generation of [^18^F]-4SFB-Avas12a1 MBs as described by Willmann et al. (2). The radiochemical yield, radiochemical purity, the SFB/Avas12a1 ratio per MB and specific activity of the final labeled product were not reported.

## In Vitro Studies: Testing in Cells and Tissues

[PubMed (http://www.ncbi.nlm.nih.gov/pubmed?term=MBs%20targeted%20to%20VEGFR2%20in%20vitro%20studies&cmd=DetailsSearch)]

No publication is currently available.

## Animal Studies

### Rodents

[PubMed (http://www.ncbi.nlm.nih.gov/pubmed?term=MBs%20targeted%20to%20VEGFR2%20Rodentia&cmd=DetailsSearch)]

The biodistribution of [^18^F]-4SFB-Avas12a1 MBs was studied in mice bearing SVR cell tumors as detailed by Willmann et al. (2). The animals (n = 4 mice; under anesthesia) were injected with 2.1 MBq (~57 μCi) of the radiolabeled MBs through the tail vein, and dynamic micro-PET imaging of the animals was initiated immediately before injection and continued for up to 60 min postinjection (p.i.) (2). The imaging data was analyzed with suitable nonproprietary software, and the amount of label accumulated in the various tissues was calculated from the images as a percentage of injected dose per gram tissue (% ID/g). The liver and spleen showed accumulation values of 34.4 ± 7.3% ID/g and 11.4 ± 10.1% ID/g, respectively, at 4 min p.i. The amount of label in the liver remained relatively constant (33.4 ± 13.7% ID/g) up to 60 min p.i., but the spleen showed a decrease in accumulated radioactivity (9.3 ± 6.5% ID/g) over this period. The peak amount of tracer in the blood was 24.5 ± 1.1% ID/g at 30 sec p.i., which decreased to 8.8 ± 0.4% ID/g at 4 min p.i. and to 0.5 ± 0.3% ID/g at 60 min p.i. The time taken to clear 50% of radioactivity from the blood was reported to be ~3.5 min. All other organs showed uptake values of <1.0% ID/g up to 60 min p.i. The tumors showed a significantly higher (P < 0.0001) accumulation of radioactivity (1.14 ± 0.41% ID/g at 4 min p.i. and 1.35 ± 0.16% ID/g at 60 min p.i.) compared to the surrounding skeletal muscles (0.84 ± 0.53% ID/g at 4 min p.i. and 0.84 ± 0.58% ID/g at 60 min p.i.). No blocking studies were reported.

To determine the in vivo stability of [^18^F]-4SFB and [^18^F]-4SFB-Avas12a1, the biodistribution of these tracers was investigated with dynamic micro-PET imaging in normal mice (n = 3 animals/radiolabeled compound) as described above (2). With the labeled Abs, a high uptake of radioactivity was observed in the liver (29.3 ± 1.9% ID/g at 4 min p.i and 30.2 ± 8.4% ID/g at 60 min p.i.) and the blood (28.5 ± 2.7% ID/g at 4 min p.i. and 20.8 ± 1.8% ID/g at 60 min p.i.). This indicated that, compared with the radiolabeled targeted MBs, the labeled Abs cleared slowly from the blood pool and stayed in circulation for at least 60 min p.i. In addition, a high accumulation of radioactivity was also observed in the kidneys (15.1 ± 4.1% ID/g at 4 min p.i. and 25.4 ± 7.7% ID/g at 60 min p.i.). After the administration of [^18^F]-4SFB the radioactivity was cleared rapidly through the kidneys (47.9 ± 3.7% ID/g at 4 min p.i. and 72.7 ± 26.3% ID/g at 60 min p.i.). The accumulation of radioactivity in the liver from the [^18^F]-4SFB was low (6.9 ± 5.2% ID/g at 4 min p.i. and 5.2 ± 2.9% ID/g) at 60 min p.i. compared to the accumulation observed with the radiolabeled MBs or [^18^F]-4SFB-Avas12a1 at the same time point.

Ex vivo biodistribution studies with the labeled MBs in nude mice (n = 3 animals/time point) showed that the trend of radioactivity uptake by the different organs of the animals was similar to that observed during the in vivo dynamic micro-PET imaging study described above (2).

From these studies, the investigators concluded that dynamic micro-PET imaging can be used to study the biodistribution of ^18^F-labeled targeted MBs in rodents (2).

### Other Non-Primate Mammals

[PubMed (http://www.ncbi.nlm.nih.gov/pubmed?term=MBs%20targeted%20to%20VEGFR2%20Other%20Non-Primate%20Mammals&cmd=DetailsSearch)]

No publication is currently available.

### Non-Human Primates

[PubMed (http://www.ncbi.nlm.nih.gov/pubmed?term=MBs%20targeted%20to%20VEGFR2%20Non-Human%20Primates&cmd=DetailsSearch)]

No publication is currently available.

## Human Studies

[PubMed (http://www.ncbi.nlm.nih.gov/pubmed?term=MBs%20targeted%20to%20VEGFR2%20Human%20Studies&cmd=DetailsSearch)]

No publication is currently available.

## Supplemental Information

[Disclaimers]

No information is currently available.

## NIH Support

These studies were supported by National Heart, Lung and Blood Institute grant 1 R01 HL078632 and National Cancer Institute grant CA114747.

## References

1 Deshpande N., Needles A., Willmann J.K. (2010). Molecular ultrasound imaging: current status and future directions. Clin Radiol.
2 Willmann J.K., Cheng Z., Davis C., Lutz A.M., Schipper M.L., Nielsen C.H., Gambhir S.S. (2008). Targeted microbubbles for imaging tumor angiogenesis: assessment of whole-body biodistribution with dynamic micro-PET in mice. Radiology.
3 Postema M., Gilja O.H. (2011). Contrast-enhanced and targeted ultrasound. World J Gastroenterol.
4 Pysz M.A., Willmann J.K. (2011). Targeted contrast-enhanced ultrasound: an emerging technology in abdominal and pelvic imaging. Gastroenterology.
5 Willmann J.K., Paulmurugan R., Chen K., Gheysens O., Rodriguez-Porcel M., Lutz A.M., Chen I.Y., Chen X., Gambhir S.S. (2008). US imaging of tumor angiogenesis with microbubbles targeted to vascular endothelial growth factor receptor type 2 in mice. Radiology.